# O-[^11^C]methyl derivative of 6,7-dimethoxy-2-(4-methoxy-biphenyl-4-yl-methyl)-1,2,3,4-tetrahydro-isoquinoline

Chemical name: | O-[^11^C]methyl derivative of 6,7-dimethoxy-2-(4-methoxy-biphenyl-4-yl-methyl)-1,2,3,4-tetrahydro-isoquinoline | [image]
Abbreviated name: | [^11^C]MC113 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | P-glycoprotein transporter | [image]
Target Category: | Transporter | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^11^C]MC113

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=p-glycoprotein%20review&cmd=DetailsSearch)]

The P-glycoprotein (P-gp) is one of the members of the ATP-binding cassette transporter family of proteins that is responsible for the rapid transportation of drugs across the cell membrane (uptake and efflux) (1). The multi-drug resistance protein and the breast cancer resistance protein (BCRP) are the other two members of this group of proteins. The structure, functions, and activities of P-gp have been discussed in detail by Giacomini et al. (2) and Sharom (3). Overexpression of these transporters, particularly P-gp, affects the distribution of drugs in various parts of the body, including the central nervous system (CNS), and this overexpression is responsible for the development of drug resistance in cancer cells (4). In addition, a reduced function and expression of P-gp has been suggested to result in a slow or reduced clearance of neurotoxic peptides such as the amyloid-β peptide from the neuronal cells, and this has been hypothesized to contribute to the development of Alzheimer’s and Parkinson’s diseases and other neurological conditions (5).

P-gp is expressed on the luminal side of the capillary endothelial cells of the blood–brain barrier (BBB) and is believed to protect the CNS from the effects of toxic compounds that may be circulating in the blood by actively pumping them from the CNS back into circulation (6). A variety of ^11^C-labeled substrates of the P-gp, such as [^11^C]verapamil, [^11^C]loperamide, and [^11^C]desmethyl loperamide, have been used with positron emission tomography (PET) to investigate the in vivo functioning of the transporter in humans (6). However, slight changes in the function or expression of P-gp that may occur in different regions of the brain may not be detected accurately with these labeled compounds because they have a low uptake in the brain (6). As an alternative to the use of labeled substrates for the detection and quantification of P-gp in the brain, it was proposed that radiolabeled inhibitors of P-gp, such as [^11^C]laniquidar, [^11^C]elacridar, and [^11^C]traiquidar, would probably yield superior results because these compounds bind to the protein with a high affinity (rather than being transported), and overexpression of the transporter would result in the generation of an increased PET signal that can be used to detect and quantify P-gp (7). Surprisingly, a very low uptake of the P-gp inhibitor probes was observed in the rodent brain; this phenomenon was attributed to the substrate-like behavior of the tracers toward the BCRP present in the organ, and this transporter was suggested to rapidly transport the radiochemicals out of the CNS across the BBB (8). Therefore, the radiolabeled inhibitors of P-gp are considered to be unsuitable to detect and determine the density of this transporter in the CNS.

In a continuing effort to develop radiolabeled inhibitors of P-gp that can be used to detect and quantify expression of the transporter in the brain, it was shown that [^11^C]MC18, a tracer containing the same basic isoquinoline structure as traiquidar and elacridar, had a four-fold higher uptake in the organ compared with [^11^C]traiquidar (9). This indicated that, compared with the other inhibitors, [^11^C]MC18 was not transported very efficiently by P-gp and/or BCRP through the BBB. In another study, it was shown that MC70 (6,7-dimethoxy-2-(4-methoxy-biphenyl-4-yl-methyl)-1,2,3,4-tetrahydro-isoquinoline), a derivative of MC18, was ~30-fold more potent than MC18 for inhibiting the P-gp–mediated transport of [^3^H]vinblastine (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=f073b58e-56d6-4c8d-a2ce-b37719402d77) (this drug interferes with the amino acid metabolic pathways of the cell) in Caco-2 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-37&Template=cellBiology) (10). On the basis of this information, Mairinger et al. synthesized and evaluated a ^11^C-labeled O-methyl derivative of MC70 ([^11^C]MC113) for the detection and measurement of P-gp expression in wild-type (WT) mice and P-gp knockout (Mdr1a/b^(–/–)^) mice (7).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5bAll+Fields%5d+AND+micad%5bbook%5d)

Protein (http://www.ncbi.nlm.nih.gov/protein/AAA59575.1) sequence of human P-gp

Information on human P-gp in Gene database (http://www.ncbi.nlm.nih.gov/gene/5243) (Gene ID: 5243)

P-gp in Online Mendelian Inheritance in Man database (OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5bAll+Fields%5d))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=P-glycoprotein&Search=Search) related to P-gp

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5BMC113%20synthesis&cmd=DetailsSearch)]

The synthesis of MC113 and its labeling with ^11^C have been described by Mairinger et al. (7). Based on the ^11^C-methane used in the reaction, the radiochemical yield of [^11^C]MC113 was 6 ± 4%. The total time required for the synthesis was ~34 min, and the radiochemical purity of the final product was >98% as determined with high-performance liquid chromatography (HPLC). The specific activity of [^11^C]MC113 at the end of synthesis was >700 GBq/μmol (>2.59 Ci/μmol). The identity of the final labeled product was confirmed with HPLC by coinjecting the tracer with a nonradioactive MC113 standard.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b11C%5dMC113%20in%20vitro%20studies&cmd=DetailsSearch)]

The expression of P-gp was determined in tumors generated with WT EMT6 cells and EMT6Ar1.0 cells in nude mice (7). The EMT6Ar1.0 cells were derived by repeated growth of EMT6 WT cells in medium supplemented with increased concentrations of doxorubicin as described elsewhere (11). The lesions were harvested from the animals at the end of the PET imaging session, and the expression of the transporter in the tumor lysates was assessed with Western blot analysis using C219, a commercially available primary anti-P-gp monoclonal antibody (7). From the Western blot analysis it was evident that the WT cell tumors had a low expression of P-gp and the transporter was overexpressed by the EMT6Ar1.0 cell lesions.

The IC_50_ values for elacridar, tariquidar, MC18, MC113, and MC70 (in increasing order) were determined with a rhodamine 123 efflux assay with CCRFvcr1000 cells (derived from CCRF-CEM cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-119&Template=cellBiology), a human T lymphoblast cell line that expresses P-gp) to be 3.2 ± 0.5 nM, 8.5 ± 2.5 nM, 351 ± 40 nM, 375 ± 60 nM, and 2,229 ± 207 nM, respectively, for these inhibitors (7). This assay indicated that MC113 did not have a very high affinity for the P-gp transporter in these cells.

A radio thin-layer chromatographic analysis of plasma obtained from WT mice at 30 min after injection of [^11^C]MC113 showed that 91 ± 2% of the radiochemical was intact at this time point (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DMC113%20rodentia&cmd=DetailsSearch)]

For PET imaging, WT mice and Mdr1a/b^(–/–)^ mice (n = 3 anesthetized animals/group) were co-injected through the tail vein with 28 ± 10 MBq (1.03 ± 0.37 mCi) [^11^C]MC113 and <0.1 nmol nonradioactive MC113 (7). Dynamic PET scans of the animals were acquired for up to 60 min postinjection (p.i.) after initiation of the tracer injection. Data were generated from the images as described elsewhere (7). For the duration of the study, the time-activity curves (TAC) of the Mdr1a/b^(–/–)^ mice were higher than those of the WT animals. A similar trend was evident for the area under the curve (AUC) values of the brain for the Mdr1a/b^(–/–)^ and the WT rodents, but the differences in the values were not statistically significant (P = 0.1).

In another study, two consecutive PET scans were acquired from nude mice bearing EMT6 cell and EMT6Ar1.0 cell tumors (n = 5 animals/group) (7). Scan 1 was started immediately after the administration of [^11^C]MC113 and lasted for 150 min p.i. At 60 min p.i. (while scan 1 was still in progress), the animals were intravenously injected with 15 mg/kg body weight nonradioactive tariquidar. Scan 2 was initiated at 120 min after the administration of nonradioactive tariquidar and lasted for 60 min. At the end of scan 2, [^18^F]fluoro-deoxyglucose was administered to the animals to define the regions of interest around the tumors, and a 20-min static scan was performed on the rodents. Although the EMT6 cell tumors and the EMT6Ar1.0 cell tumors were clearly visible in the PET images, the TACs with [^11^C]MC113 were higher in the EMT6 lesions than in the EMT6Ar1.0 tumors in both scans. No significant difference was noticed in the AUC values for both the tumor types (AUC_0–60_, scan 1: EMT6: 76 ± 19 min, EMT6Ar1.0: 65 ± 6 min, P = 0.313; AUC_0–60_, scan 2: EMT6: 90 ± 23 min, EMT6Ar1.0: 69 ± 8 min, P = 0.063, Wilcoxon matched-pairs signed rank test). The peak uptake of radioactivity in the brain of the animals (~1.7 standardized uptake value (SUV) at 9 min p.i.) was comparable with that of the tumors (~1.5 SUV at 9 min p.i.). However, during the course of the study, the label cleared rapidly from the brain, while the tracer continued to accumulate in the tumor during the period. No significant difference in the brain AUC values was observed between the two scans (P = 0.063).

From these studies, it is apparent that the accumulation of radioactivity from [^11^C]MC113 in the brain was due to a reduced transport of the tracer by the P-gp and/or the BCRP in the BBB (7). The signal obtained from the BBB and the tumors was probably due to nonspecific binding of radioactivity because MC113 was observed to have a low affinity for P-gp as determined with the rhodamine 123 efflux assays. Therefore, the investigators concluded that [^11^C]MC113 was not suitable for the visualization of P-gp expression in the CNS and the cancerous lesions of rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DMC113%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DMC113%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DMC113%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Haar C.P., Hebbar P., Wallace G.C.t., Das A., Vandergrift W.A., Smith J.A., Giglio P., Patel S.J., Ray S.K., Banik N.L. (2012). Drug resistance in glioblastoma: a mini review. Neurochem Res.
2 Giacomini K.M., Huang S.M., Tweedie D.J., Benet L.Z., Brouwer K.L., Chu X., Dahlin A., Evers R., Fischer V., Hillgren K.M., Hoffmaster K.A., Ishikawa T., Keppler D., Kim R.B., Lee C.A., Niemi M., Polli J.W., Sugiyama Y., Swaan P.W., Ware J.A., Wright S.H., Yee S.W., Zamek-Gliszczynski M.J., Zhang L. (2010). Membrane transporters in drug development. Nat Rev Drug Discov.
3 Sharom F.J. (2011). The P-glycoprotein multidrug transporter. Essays Biochem.
4 Hitchcock S.A. (2012). Structural modifications that alter the P-glycoprotein efflux properties of compounds. J Med Chem.
5 Bartels A.L. (2011). Blood-brain barrier P-glycoprotein function in neurodegenerative disease. Curr Pharm Des.
6 Luurtsema G., Verbeek G.L., Lubberink M., Lammertsma A.A., Dierckx R., Elsinga P., Windhorst A.D., van Waarde A. (2010). Carbon-11 labeled tracers for in vivo imaging P-glycoprotein function: kinetics, advantages and disadvantages. Curr Top Med Chem.
7 Mairinger S., Wanek T., Kuntner C., Doenmez Y., Strommer S., Stanek J., Capparelli E., Chiba P., Muller M., Colabufo N.A., Langer O. (2012). Synthesis and preclinical evaluation of the radiolabeled P-glycoprotein inhibitor [(11)C]MC113. Nucl Med Biol.
8 Kannan P., Telu S., Shukla S., Ambudkar S.V., Pike V.W., Halldin C., Gottesman M.M., Innis R.B., Hall M.D. (2011). The "Specific" P-Glycoprotein Inhibitor Tariquidar Is Also a Substrate and an Inhibitor for Breast Cancer Resistance Protein (BCRP/ABCG2). ACS Chem Neurosci.
9 van Waarde A., Ramakrishnan N.K., Rybczynska A.A., Elsinga P.H., Berardi F., de Jong J.R., Kwizera C., Perrone R., Cantore M., Sijbesma J.W., Dierckx R.A., Colabufo N.A. (2009). Synthesis and preclinical evaluation of novel PET probes for P-glycoprotein function and expression. J Med Chem.
10 Colabufo N.A., Berardi F., Cantore M., Perrone M.G., Contino M., Inglese C., Niso M., Perrone R., Azzariti A., Simone G.M., Paradiso A. (2008). 4-Biphenyl and 2-naphthyl substituted 6,7-dimethoxytetrahydroisoquinoline derivatives as potent P-gp modulators. Bioorg Med Chem.
11 Wanek T., Kuntner C., Bankstahl J.P., Bankstahl M., Stanek J., Sauberer M., Mairinger S., Strommer S., Wacheck V., Loscher W., Erker T., Muller M., Langer O. (2012). A comparative small-animal PET evaluation of [11C]tariquidar, [11C]elacridar and (R)-[11C]verapamil for detection of P-glycoprotein-expressing murine breast cancer. Eur J Nucl Med Mol Imaging.